# ^99m^Tc-Labeled tumor-associated glycoprotein 72 binding peptides A2-6 and A3-10

Chemical name: | ^99m^Tc-Labeled tumor-associated glycoprotein 72 binding peptides A2-6 and A3-10
Abbreviated name: | [^99m^Tc]-A2-6 and [^99m^Tc]-A3-10
Synonym:
Agent Category: | Peptides
Target: | Tumor-associated glycoprotein 72
Target Category: | Other (glycoprotein)
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TAG-72&cmd=DetailsSearch)]

The tumor-associated glycoprotein 72 (TAG-72) is a high molecular weight mucigenous protein that is found mainly in the extracellular matrix of neoplastic tumors (1). This glycoprotein is usually not expressed in normal tissues but is overexpressed in the tumors of several cancers, such as those of the colon and rectum (colorectal cancer), stomach, pancreas, ovaries, prostate, lung, breast, etc. Therefore, TAG-72 is considered to have much theranostic value (useful for the diagnosis and/or therapy of a disease) because it can be used for antigen-directed surgical resection of cancerous tumors with radiolabeled anti-TAG-72 monoclonal antibodies (mAb) (1). In addition, the detection or absence of TAG-72 expression in colorectal cancer tumors was shown to have prognostic value because individuals who had complete removal of tumors with surgery guided by mouse anti-Tag-72 mAb were shown to have a long-term survival advantage compared to patients who had an incomplete removal of the lesions (2). However, the main limitation of using radiolabeled antibodies (Ab) or their fragments to detect and treat malignant tumors is the long circulation half-life of these molecules and the development of human anti-mouse antibodies in the patients (3). In comparison, synthetic anti-tumor peptides that can be used for the noninvasive imaging and therapy of cancers show rapid clearance from circulation and non-target tissue, have more access and deeper penetration into the lesions, and may not be immunogenic (3-5).

Recently, the peptides GGVSCMQTSPVCENNL (A2-6) and NPGTCKDKWEICLLNGG (A3-10) were identified from a phase-display peptide library (f88-4/cys6) against TAG-72 and labeled with ^99m^Tc to generate [^99m^Tc]-A2-6 and [^99m^Tc]-A3-10 (4). The labeled peptides were then evaluated in mice for the detection of LS-174T cell (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CL-188&Template=cellBiology) xenograft tumors that overexpress the TAG-72 antigen in mice. In another study, a modified procedure (from that used to purify the A2-6 and A3-10 peptides) was used to purify peptides from the f88-4/cys6 phage library, and two new peptides, FRERCDKHPQKCTKFL (G3-15) and DPRHCQKRVLPCPAWL (T3-15), that had a high affinity for the TAG-72 antigen were identified (3). These peptides were then labeled with ^99m^Tc to obtain [^99m^Tc]-G3-15 and [^99m^Tc]-T3-15, and the labeled compounds were tested for the detection of LS-174T cell xenograft tumors in mice. This chapter describes the results obtained with [^99m^Tc]-A2-6 and [^99m^Tc]-A3-10. Studies performed with [^99m^Tc]-G3-15 and [^99m^Tc]-T3-15 are described in a separate chapter of MICAD (www.micad.nih.gov) (6).

### Related Resource Links

TAG-72 related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=TAG-72+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=TAG-72) related to TAG-72

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Synthesis%20of%20TAG-72%20binding%20peptides&cmd=DetailsSearch)]

Peptides A3-6 and A3-10 were obtained in their native L-configuration from a commercial source, biotinylated, conjugated with N-hydroxysuccinimidyl-S-acetyl-mercaptoacetyltriglycine, and labeled with ^99m^Tc as described by Chen et al. (4). The peptides were purified on a Biogel P2 size-exclusion column and had a radiochemical purity of >90% as determined with instant thin-layer chromatography, paper chromatography, and reversed-phase high-performance liquid chromatography (4). The radiochemical yields of the labeled peptides were not reported. The specific activity of the peptides was reported to be 1.68 MBq/nmol (45.36 μCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TAG-72%20binding%20peptides%20in%20vitro%20studies&cmd=DetailsSearch\)]

Cell binding of the biotinylated peptides was determined with flow cytometry analysis as described by Chen et al. (4). Briefly, LS-174T cells (overexpress TAG-72) and HT-29 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-38&Template=cellBiology) (controls; do not express TAG-72) were respectively incubated with increasing concentrations of the peptides, washed to remove the excess peptides, and treated with a mouse anti-biotin Ab. Subsequently, Phycoerythrin anti-mouse Ab was used to detect the cell-bound peptides with flow cytometry. Only the LS-174T cells were observed to bind the peptides, indicating a cell-binding specificity of the compounds.

The IC_50_ values of the two ^99m^Tc-labeled peptides were determined in an in vitro competitive binding assay (4). The LS-174T cells were incubated with the labeled peptides in the presence of increasing concentrations (10−^12^ to 10−^4^ mol/L) of the respective non-labeled peptides, and the IC_50_ values were calculated as described by Chen et al. (4). The IC_50_ values of A2-6 and A3-10 were determined to be 46.5 nmol/L and 420 nmol/L, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TAG-72%20binding%20peptides%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^99m^Tc]-A2-6 and [^99m^Tc]-A3-10 was investigated in mice (n = 2–3 animals/group) bearing LS-174T cell tumors on the left shoulder (4). The animals were anesthetized during imaging and injected with 20 μg, 1.68 MBq/nmol (45.36 μCi/nmol), of the labeled peptide through the tail vein. A computed tomography (CT) scan was acquired 20 min after injection. This was followed by two sequential single-photon emission computed tomography (SPECT) whole-body scans at 30 min and 60 min postinjection (p.i.). Volumes of interest (VOIs) were drawn around the tumor and the normal organs in all the images, and the percent injected dose (% ID) was calculated using appropriate software as described elsewhere (4). The tumors in the mice were visible with both radiolabeled peptides at 30 min and 60 min p.i., but they were no longer visible at 3 h p.i. (data not presented). With [^99m^Tc]-A3-10, the accumulation of radioactivity in the tumor was 1.4% ID at 30 min p.i. compared with 0.6% ID for [^99m^Tc]-A2-6 at the same time point. The highest label accumulation was observed in the kidneys, followed by the gallbladder and the intestines at 30 min p.i. Little uptake of radioactivity was observed in the other organs. A high level of radioactivity was also observed in the liver with [^99m^Tc]-A2-6.

In another study, pre-injection of the animals with unlabeled A3-10 peptide (100 μg/animal) was shown to block 80% of the uptake of radioactivity from [^99m^Tc]-A3-10 by the LS-174T cell tumors (4). In addition, the presence of excess unlabeled peptide did not block the accumulation of label in the normal organs. These observations indicate that the A3-10 peptide binds specifically to cells that overexpress the TAG-72 antigen in the xenograft tumors.

From these studies, the investigators concluded that the A3-10 peptide, although it had lower cell-binding affinity for the TAG-72 antigen compared to the A2-6 peptide, exhibited higher accumulation in tumors expressing the TAG-72 antigen and should be evaluated further as a potential imaging agent for TAG-72–positive cancers (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TAG-72%20binding%20peptides%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TAG-72%20binding%20peptides%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TAG-72%20binding%20peptides%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

## NIH Support

Studies reported in this chapter were supported by a National Institutes of Health grant CA111606.

## References

1 Povoski S.P., Hatzaras I.S., Mojzisik C.M., Martin E.W. (2011). Oncologic theranostics: recognition of this concept in antigen-directed cancer therapy for colorectal cancer with anti-TAG-72 monoclonal antibodies. Expert Rev Mol Diagn.
2 Povoski, S.P., I.S. Hatzaras, C.M. Mojzisik, M.W. Arnold, G.H. Hinkle, C.L. Hitchcock, D.C. Young, and E.W. Martin, Jr., Antigen-Directed Cancer Surgery for Primary Colorectal Cancer: 15-Year Survival Analysis. Ann Surg Oncol, 2011
3 Xiao N., Cheng D., Wang Y., Chen L., Liu X., Dou S., Liu G., Liang M., Hnatowich D.J., Rusckowski M. (2011). Identification of a high affinity TAG-72 binding peptide by phage display selection. Cancer Biol Ther.
4 Chen L., Wang Y., Cheng D., Dou S., Liu X., Liu G., Hnatowich D.J., Rusckowski M. (2011). Comparing two TAG-72 binding peptides previously identified by phage display as potential imaging agents. Nucl Med Commun.
5 Rusckowski M., Gupta S., Liu G., Dou S., Hnatowich D.J. (2007). Evidence of specificity of radiolabeled phage display peptides for the TAG-72 antigen. Cancer Biother Radiopharm.
6 Chopra, A., 99mTc-Labeled tumor-associated glycoprotein 72 binding peptides, G3-15 and T3-15. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.